# 2-[(4-{[(2-amino-4-oxohydropteridin-7yl)methyl]amino}phenyl) carbonylamino]-4-{N-[(2-[18F]-fluoro(4-pyridyl))carbonylamino] carbamoyl}butanoic acid

Chemical name: | 2-[(4-{[(2-amino-4-oxohydropteridin-7yl)methyl]amino}phenyl) carbonylamino]-4-{N-[(2-[^18^F]-fluoro(4-pyridyl))carbonylamino] carbamoyl}butanoic acid
Abbreviated name: | [^18^F]-Folate-2
Synonym: | [^18^F]-2-fluoropyridine-4-carbohydrazide-folate; [^18^F]-2; [^18^F]-9
Agent Category: | Compound
Target: | Folate receptor
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on above structure for information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=folate%20receptor%20imaging&cmd=DetailsSearch)]

Folic acid (FA; also known as folate or vitamin B_9_) is a water-soluble vitamin that is required for the synthesis and repair of DNA in the cell. FA also acts as a cofactor for many biological reactions and has an important role in cell maintenance and proliferation. Although the folate receptor (FR) is expressed at low levels in normal cells, this receptor is known to be upregulated in cancers such as those of the ovary, lung, breast, brain, colon, and the hematopoietic lineage cells (1). Therefore, the FR system has been targeted with radiolabeled folate and its derivatives, such as ^67^Ga-deferoxamine (DF)-folate, ^111^In-diethylenetriamine pentaacetic acid-folate, ^99m^Tc-mercaptoacetyldiglycine-folate-methotrexate, etc., for the noninvasive detection of malignancies with single-photon emission computed tomography (2). Mathias et al. showed that ^66/67^Ga-DF-folate can be used with positron emission tomography (PET) for the imaging of FR-positive cancerous tumors in mice (3). However, although these tracers could detect the FR-rich tumors, they were deemed unsuitable for imaging lesions in the abdominal regions because high levels of radioactivity were observed to accumulate in the liver and the intestines of the animals (4). In addition, ^66/67^Ga-labeled tracers are known to produce low-resolution images due to their high positron energy (4.15 MeV and 1.89 MeV for ^66^Ga and ^67^Ga, respectively. ^67^Ga-labeled agents are used for single photon emission computed tomography imaging) compared to ^18^F (0.64 MeV), which generates superior images and is often used to radiolabel PET imaging agents in the clinic (4). In another study, it was shown that ^18^F-fluorobenzylamine derivatives of folate can detect tumors that had a high expression of FR, but the radioactivity from these labeled compounds accumulated mainly at the rim of the tumor, and large amounts of the label were retained in the liver and intestines of the animals (4, 5).

In an ongoing effort to generate radiolabeled agents for the imaging of tumors that express high levels of FRs that would be superior to those developed and evaluated earlier, a ^18^F-fluorobenzene derivative of folic acid ([^18^F]-folate-1), a pyridinecarbohydrazide-folate derivative of folic acid ([^18^F]-folate-2), a ^18^F-fluorobenzene/methotrexate (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=78794e3d-f293-4eeb-22ac-8f536d5947eb) (MTX) conjugate of folic acid ([^18^F]-folate-MTX-8), and a ^18^F-pyridinecarbohydrazide-folate/methotrexate conjugate of folic acid ([^18^F]-folate-MTX-9) have been synthesized (2). The biodistribution of these tracers was investigated in healthy mice. On the basis of results obtained from these studies, [^18^F]-folate-2 was evaluated for the PET imaging of human KB cell line (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CCL-17&Template=cellBiology) xenograft tumors (have a high expression of FR) in mice. This chapter describes the results obtained with [^18^F]-folate-2. Separate chapters in MICAD (http://www.micad.nih.gov/) discuss the studies performed with [^18^F]-folate-1 (6), [^18^F]-folate-MTX-8 (7), and [^18^F]-folate-MTX-9 (8).

### Related Resource Links

FR-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Folate+receptor+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Adult human FR protein and mRNA sequences (http://www.ncbi.nlm.nih.gov/nuccore/NM_016724.2)

Human FR gene (http://www.ncbi.nlm.nih.gov/gene/2348) (Gene ID: 2348)

FR clinical trials (http://clinicaltrials.gov/ct2/results?term=folate+receptor+AND+targeted+AND+cancer)

FR in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim/136430) database

FR pathway in Kyoto Encyclopedia of Genes and Genomes (KEGG) (http://www.genome.jp/dbget-bin/www_bget?hsa:2348+hsa:2350+hsa:2352+hsa:390243)

Folic acid information on Dailymed site (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=ff80ef4d-e04c-9f83-2b56-cccc30028f72)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-F-1%20synthesis&cmd=DetailsSearch)]

Folate-2 was synthesized with 2,5-dioxoazolidinyl 2-fluoropyridine-4-carboxylate and hydrazide-folate in presence of triethylamine. The ^18^F labeling of folate-2 is detailed elsewhere (9). The synthesis of [^18^F]-folate-1 is described in (6). The total time of synthesis for each of the tracers was ~45 min, and the radiochemical yield and radiochemical purity of both the final labeled products were >80% (based on the initial ^18^F concentration) and >97% (without high-performance liquid chromatographic purification), respectively. The specific activity of each of the radiolabeled compounds was reported to be >11.11 MBq/μmol (300 mCi/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-F-1%20in%20vitro&cmd=DetailsSearch)]

Using an n-octanol-water mixture (pH 7.3), the partition coefficients of [^18^F]-folate-2 and [^18^F]-folate-1 were determined to be 0.14 ± 0.01 and 0.38 ± 0.02, respectively, indicating that the labeled compounds had a low lipophilicity (9).

Both [^18^F]-folate-2 and [^18^F]-folate-1 were reported to be stable in human plasma for at least 4 h at 37°C (data not presented) (2).

The FR binding affinities of [^18^F]-folate-2 and [^18^F]-folate-1 were determined to be 15.51 ± 1.80 nM and 13.08 ± 0.83 nM, respectively, with a saturation assay using KB cell membranes (9). A cell internalization assay of [^18^F]-folate-2 and [^18^F]-folate-1 with KB cells (using an acidic buffer, pH not mentioned) showed that 11.86 ± 0.43% and 25.85 ± 0.95% of the tracers was respectively internalized by the cells within 20 min at 37°C.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-F-1%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^18^F]-folate-2 and [^18^F]-folate-1 was studied in normal Balb/c mice as described by Jammaz et al. (2). The animals (n = 4 mice/time point for each tracer) were injected with 749 kBq (20 μCi) of the tracer through the tail vein and euthanized at 10, 60, and 120 min postinjection (p.i.) to determine the amount of radioactivity accumulated in the various organs. All data were presented as percent of injected dose per gram tissue (% ID/g). Radioactivity from [^18^F]-folate-2 was rapidly cleared from the blood (1.22 ± 0.61% ID/g at 10 min p.i., 0.10 ± 0.05% ID/g at 60 min p.i., and 0.04 ± 0.01% ID/g at 120 min p.i.). High amounts of label accumulated in the kidneys (13.8 ± 5.9% ID/g at 10 min p.i. and 2.92 ± 0.51% ID/g at 120 min p.i.), and low levels of radioactivity were detected in the intestine (0.76 ± 0.20% ID/g at 10 min p.i. and 0.03 ± 0.01% ID/g at 120 min p.i.). This indicated that the tracer was excreted primarily through the urinary route. With [^18^F]-folate-1, rapid clearance of radioactivity from the blood was observed (4.41 ± 0.60% ID/g at 10 min p.i., 2.55 ± 1.50% ID/g at 60 min p.i., and 1.13 ± 0.51% ID/g at 120 min p.i.). High levels of [^18^F]-folate-1 were observed in the kidneys (22.50 ± 4.42% ID/g at 10 min p.i. and 17.88 ± 0.10% ID/g at 120 min p.i.) and the intestine (5.95 ± 2.11% ID/g at 10 min p.i. and 5.86 ± 0.26% ID/g at 120 min p.i.) of these animals, indicating that the tracer was excreted through the urinary and the hepatobiliary routes. The low accumulation of radioactivity with [^18^F]-folate-2 in the various organs suggested that this tracer had superior pharmacokinetics compared to [^18^F]-folate-1.

The biodistribution of [^18^F]-folate-2 and [^18^F]-folate-1 was also investigated in nude mice (n = 4 animals/tracer) bearing KB cell tumors (2). The animals were injected with the radiotracers as described above and euthanized at 60 min p.i. With both radiolabeled compounds, the uptake of radioactivity in the various organs of the mice at 60 min p.i. was similar to that observed earlier (see above). The amount of tumor accumulation with [^18^F]-folate-2 and [^18^F]-folate-1 at 60 min p.i. was 5.74 ± 0.16% ID/g and 5.94 ± 1.16% ID/g, respectively, indicating that with both tracers there was a similar uptake of radioactivity in the tumors. The tumor/blood and tumor/muscle ratios at 60 min p.i. were 14.70 and 28.70, respectively, with [^18^F]-folate-2 and 6.39 and 25.83, respectively, with [^18^F]-folate-1. For blocking studies, the mice were injected with 100 μg (0.22 μmol) FA 10 min before the administration of either [^18^F]-folate-2 or [^18^F]-folate-1, and the rodents were subsequently treated as before (2). With [^18^F]-folate-2, the uptake of radioactivity in the tumor at 60 min p.i. was reduced to 0.66 ± 0.10% ID/g (P < 0.05), and a similar trend was observed in the kidneys, liver, and intestines (P < 0.05); among these organs only the kidneys and the liver show high expression of Fr compared with other normal tissues. After pretreatment with FA, the uptake of radioactivity from [^18^F]-folate-1 in the tumors at 60 min p.i. was reduced significantly (0.74 ± 0.17% ID/g, P < 0.05); the kidneys, liver and intestines also showed a reduced uptake of the label (P < 0.05) at 60 min p.i. This indicated that both [^18^F]-folate-2 and [^18^F]-folate-1 had a high binding specificity for the FR in the tumors and the various organs.

From the studies and the results discussed above, the investigators concluded that [^18^F]-folate-2 was probably superior to [^18^F]-folate-1 for the imaging of FR-expressing tumors (2). Nude mice (number not reported) bearing KB cell tumors were injected with 11–18.5 MBq (300–500 μCi) [^18^F]-folate-2 through the tail vein, and whole-body PET images of the animals (under anesthesia) were acquired 45 min p.i. From the images it was clear that radioactivity from [^18^F]-folate-2 was present primarily in the kidneys, bladder, and the tumor of the animals. No other organ or tissues of the mice were visible in the images. No blocking studies for in vivo imaging were reported.

Table: Tumor Uptake and Tumor/Blood and Tumor/Muscle Ratios of different ^ 18 ^ F-Labeled Folates

Tracer | Tumor Uptake (% ID/g) | | Ratio (No Folate Pre-treatment)
Tracer | No Folate Pre-treatment | With Folate (100 μg) Pre-treatment | Tumor/blood | Tumor/Muscle
[ ^ 18 ^ F]-Folate-1 | 5.94 ± 1.16 | 0.74 ± 0.17 | 6.39 | 25.83
[ ^ 18 ^ F]-Folate-2 | 5.74 ± 0.16 | 0.66 ± 0.10 | 14.72 | 28.70

From these studies, the investigators concluded that [^18^F]-folate-2 was probably a suitable PET imaging agent for the visualization of FR-rich tumors in rodents (2).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-F-1%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-F-1%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-F-1%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Xia W., Low P.S. (2010). Folate-targeted therapies for cancer. J Med Chem.
2 Al Jammaz I., Al-Otaibi B., Amer S., Okarvi S.M. (2011). Rapid synthesis and in vitro and in vivo evaluation of folic acid derivatives labeled with fluorine-18 for PET imaging of folate receptor-positive tumors. Nucl Med Biol.
3 Mathias C.J., Lewis M.R., Reichert D.E., Laforest R., Sharp T.L., Lewis J.S., Yang Z.F., Waters D.J., Snyder P.W., Low P.S., Welch M.J., Green M.A. (2003). Preparation of 66Ga- and 68Ga-labeled Ga(III)-deferoxamine-folate as potential folate-receptor-targeted PET radiopharmaceuticals. Nucl Med Biol.
4 Sega E.I., Low P.S. (2008). Tumor detection using folate receptor-targeted imaging agents. Cancer Metastasis Rev.
5 Bettio A., Honer M., Muller C., Bruhlmeier M., Muller U., Schibli R., Groehn V., Schubiger A.P., Ametamey S.M. (2006). Synthesis and preclinical evaluation of a folic acid derivative labeled with 18F for PET imaging of folate receptor-positive tumors. J Nucl Med.
6 Chopra, A., 2-[(4-{[(2-amino-4-oxohydropteridin-7yl)methyl]amino}phenyl) carbonylamino]-4-{N-[(4-[18F]-fluorophenyl)carbonylamino] carbamoyl}butanoic acid. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
7 Chopra, A., 2-[(4-{[(2-amino-4-oxohydropteridin-7yl)methyl]amino}phenyl) carbonylamino]-4-{N-[(2-[18F]-fluoro(4-pyridyl))carbonylamino] carbamoyl}butanoic acid. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
8 Chopra, A., 2-[18F]Fluoropyridine-4-carbohydrazide-methotrexate (9). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
9 Jammaz I.A., Otaibi B.A., Okarvi S., Amartey J.K. (2006). Novel synthesis of [18F]-fluorobenzene and pyridinecarbohydrazide-folates as potential PET radiopharmaceuticals. Journal of Labelled Compounds and Radiopharmaceuticals.